# ^89^Zr-Desferrioxamine-anti-epithelial glycoprotein-1 hRS7 humanized monoclonal antibody

Chemical name: | ^89^Zr-Desferrioxamine-anti-epithelial glycoprotein-1 hRS7 humanized monoclonal antibody
Abbreviated name: | ^89^Zr-Df-hRS1
Synonym:
Agent category: | Antibody
Target: | Epithelial glycoprotein-1 (EGP-1, also known as TROP2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/ contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/ACR78188.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002353.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4070) for more information about EGP-1

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7)]

Epithelial glycoprotein-1 (EGP-1, also known as TROP2) is a transmembrane glycoprotein (46 kDa) identified with murine IgG_1_ monoclonal antibody (mAb) RS7 raised against human non-small cell lung carcinoma (1). EGP-1 is also present in human carcinomas of the stomach, bladder, breast, ovary, uterus, and prostate, but it is not expressed in most normal tissues. EGP-1 is expressed at low levels in glandular cells in the bronchus, breast, prostate, skin, and pancreas. EGP-1 activates intracellular calcium mobilization (2) and protein kinase C (3) after binding with RS7. EGP-1 is a cell-surface receptor with unknown physiological ligand and cellular functions. However, EGP-1 has been implicated in the activation of the ERK/MAPK pathway, leading to downstream alterations in cellular proliferation, migration, invasion, and survival of cancer cells (4). EGP-1 overexpression has been associated with increased tumor invasiveness and decreased overall survival rates in multiple types of human carcinomas (5, 6). van Rij et al. (7) evaluated ^89^Zr-desferrioxamine-hRS7 (^89^Zr-Df-hRS7) as a ^89^Zr-based positron emission tomography (PET) agent in human prostate PC-3 tumors in nude mice.

### Related Resource Links:

- Chapters in MICAD (EGP-1 (http://www.ncbi.nlm.nih.gov/books?term=(EGP-1%20OR%20EpCAM)%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGP-1 (http://www.ncbi.nlm.nih.gov/gene/4070))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGP-1 (http://www.ncbi.nlm.nih.gov/omim/137290))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+synthesis)]

Df-hRS7 was prepared by conjugation of N-succinyldesferrioxamine tetrafluorophenol to hRS7 for 30 min at 25°C. Df-hRS7 was purified with column chromatography (7). There was one Df moiety per mAb. Df-hRS7 was incubated with ^89^Zr-oxalate in HEPES buffer (pH 7) for 90 min at 25°C. ^89^Zr-Df-hRS7 was purified with column chromatography. This procedure provided a radiolabeling yield of 60%, with a specific activity of 82 MBq/nmol (2.2 mCi/nmol) and a radiochemical purity of >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+in+vitro)]

Immunostaining of PC-3 tumor sections with hRS7 showed the expression of EGP-1 in the membranes and cytosol of PC-3 tumor cells (7). Immunochemical analysis of three human primary prostate tumor sections showed high homogeneous and consistent expression of EGP-1 in all three tumors and metastases in a lymph node and in the liver. The immunoreactivity of ^89^Zr-Df-hRS7 was >80%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+in+vitro)]

van Rij et al. (7) injected 11 MBq (0.3 mCi (0.13 nmol)) ^89^Zr-Df-hRS7 into male nude mice (n = 5) bearing the EGP-1–positive PC-3 prostate tumors for PET imaging at 1, 3, and 7 d. PET imaging estimated tumor accumulation of 31%, 46%, and 55% injected dose/gram (ID/g) at 1, 3, and 7 d after injection of ^89^Zr-Df-hRS7, respectively. The radioactivity in the blood was 16% ID/g at 1 d and declined to 6% ID/g at 7 d. The tumors were clearly visualized at 3 d and 7 d. There was little accumulation in the other organs except the femur (~3% ID/g at 3 d and ~10% ID/g at 7 d). The tumor/liver ratios were 2.9, 6.5, and 7.7 at 1, 3, and 7 d, respectively. Co-injection of excess hRS7 (3.3 nmol) inhibited accumulation in the tumors to 10% ID/g at 3 d after injection. Little inhibition was observed in the other organs, including the femur. The imaging studies were not confirmed by ex vivo biodistribution.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+human)]

No publication is currently available.

## References

1 Stein R., Chen S., Sharkey R.M., Goldenberg D.M. (1990). Murine monoclonal antibodies raised against human non-small cell carcinoma of the lung: specificity and tumor targeting. Cancer Res.
2 Ripani E., Sacchetti A., Corda D., Alberti S. (1998). Human Trop-2 is a tumor-associated calcium signal transducer. Int J Cancer.
3 Basu A., Goldenberg D.M., Stein R. (1995). The epithelial/carcinoma antigen EGP-1, recognized by monoclonal antibody RS7-3G11, is phosphorylated on serine 303. Int J Cancer.
4 Cubas R., Zhang S., Li M., Chen C., Yao Q. (2010). Trop2 expression contributes to tumor pathogenesis by activating the ERK MAPK pathway. Mol Cancer.
5 Varughese J., Cocco E., Bellone S., de Leon M., Bellone M., Todeschini P., Schwartz P.E., Rutherford T.J., Pecorelli S., Santin A.D. (2011). Uterine serous papillary carcinomas overexpress human trophoblast-cell-surface marker (Trop-2) and are highly sensitive to immunotherapy with hRS7, a humanized anti-Trop-2 monoclonal antibody. Cancer.
6 Bignotti E., Todeschini P., Calza S., Falchetti M., Ravanini M., Tassi R.A., Ravaggi A., Bandiera E., Romani C., Zanotti L., Tognon G., Odicino F.E., Facchetti F., Pecorelli S., Santin A.D. (2010). Trop-2 overexpression as an independent marker for poor overall survival in ovarian carcinoma patients. Eur J Cancer.
7 van Rij C.M., Sharkey R.M., Goldenberg D.M., Frielink C., Molkenboer J.D., Franssen G.M., van Weerden W.M., Oyen W.J., Boerman O.C. (2011). Imaging of prostate cancer with immuno-PET and immuno-SPECT using a radiolabeled anti-EGP-1 monoclonal antibody. J Nucl Med.